# Biotinylated anti-Tn MLS128 monoclonal antibody-^125^I-streptavidin

Chemical name: | Biotinylated anti-Tn MLS128 monoclonal antibody-^125^I-streptavidin
Abbreviated name: | Bt-MLS128-^125^I-SA
Synonym:
Agent Category: | Antibody
Target: | Tumor-associated carbohydrate Tn antigen
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=PureSearch&db=pubmed&term=%22Tn%20antigen%22)]

Tn antigen is a tumor-associated carbohydrate epitope (N-acetyl-galactosamine (GalNAc)-O-Ser/Thr (GalNAca-O-Ser/Thr)) (1-3). Two-step targeting with biotinylated MLS128 murine monoclonal antibody (Bt-MLS128 mAb) and ^125^I-labeled streptavidin (^125^I-SA) was developed for in vivo imaging of Tn antigen-expressing tumors (4-7). It was designed on the basis of avidin’s extraordinarily high binding affinity for biotin.

Avidin’s high affinity for biotin was first exploited in histochemical applications in the mid-1970s (8, 9). This affinity is more than one million times higher than that of most antibodies for most antigens. Avidin has four binding sites for biotin, and most proteins, including enzymes, can be conjugated with several molecules of biotin. The avidin-biotin binding is essentially irreversible. These properties allow molecular complexes to be formed between avidin and biotinylated antibodies. In addition, small molecular sizes of avidin and biotin allow improved tumor uptake and rapid intratumoral spatial distribution.

Altered glycosylation on the cell surface is a hallmark of malignant transformation and tumor progression. Incomplete synthesis of the carbohydrate chains and precursor accumulation result in loss of the normal carbohydrate antigens and high expression of the tumor-associated carbohydrate antigens (10-12). Lewis Y, TF, Globo H, GM2, polysialic acid, sialyl Lewis A, Tn, and sialyl Tn are some of the antigens investigated intensively as diagnostic markers or as vaccine antigens (11-14). Tn antigen was first reported as a tumor-associated antigen nearly 40 years ago (15). It is composed of a single GalNAc glycan residue attached via an α-linkage to either the serine (Ser) or the threonine (Thr) of a polypeptide chain (12, 14). In normal tissues, Tn antigen is masked by covalently bound terminal carbohydrate moieties, but in tumors it is unmasked because of defective O-glycosylation. Accordingly, Tn antigen is rarely expressed in normal tissues, but it is widely expressed in human carcinomas or hematological cancers. It has been reported that the Tn antigen is expressed in 70–90% of breast, colon, lung, bladder, cervical, ovarian, stomach, and prostate tumors (1, 3, 10). The expression levels of Tn antigen are closely associated with tumor aggressiveness and poor survival of patients (11, 13). In addition, Tn antigen is recognized by the human immune system as a novel epitope, provoking immune responses in patients. There is a significant correlation among the expression of the Tn antigen, the development of the spontaneous antibodies against Tn, and the prognosis for patients with carcinomas. Clinical trials are under way to deliberately provoke or enhance human immune responses by injecting patients with synthetic peptide antigens bearing Tn structure (3, 11, 16-18). Tn antigen has attracted significant interest as a target for tumor diagnosis and immunotherapy. A number of anti-Tn IgG and IgM antibodies have been generated and investigated for their imaging feasibilities and anti-tumor activities (2, 4, 5, 19-24). The results are generally inconsistent. There are still some issues to be resolved, such as immunogenicity, reduced effectiveness in vivo, and cross-reactivity against type-A blood antigen. In addition, directly radiolabeled antibodies usually show a slow and low accumulation in tumors, and their blood clearance is also slow. Zhang et al. tested the imaging feasibility of two-step targeting with Bt-MLS128 and ^125^I-SA in mice bearing LS180 human colon cancer xenografts (4).

Note: Investigators from the same research group as Zhang et al. also labeled the anti-Tn MLS128 mAb directly with ^125^I/^131^I (^125^I/^131^I-MLS128 (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) and ^111^In (^111^In-MLS128 (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)), separately, and investigated their biodistribution and the feasibility of imaging tumors in mice bearing LS180 tumor xenografts. They also tested the imaging feasibility of three-step targeting with Bt-MLS128, SA, and ^111^In-DTPA-biotin (Bt-MLS128-SA-^111^In-biotin (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) in mice with LS180 tumor xenografts (4-7, 20).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Imaging with two-step targeting included two agents: Bt-MLS128 and ^125^I-SA (4, 5, 22). Bt-MLS128 served as the binding site for the ^125^I-SA. The anti-Tn MLS128 is a mouse IgG3 antibody with κ light chain, and it is produced by immunizing mice with LS180 human colorectal cancer cells (23). The murine OST6 mAb against an alkaline phosphatase-related substance was used as the control. The antibodies were biotinylated by mixing them with sulfosuccinimidyl-6-(biotinamido)hexanoate. The biotinylated antibodies were purified with chromatography on PD-10 gel. The average numbers of biotin molecules coupled to the MLS128 and the OST6 were 1.2 and 1.7, respectively. Bt-MLS128, Bt-OST6, and SA were also radioiodinated with ^125^I with the chloramine-T method. The labeling efficiencies of radioiodinated Bt-MLS128 (^125^I-Bt-MLS128), Bt-OST6, and SA were 63.2, 58.3, and 81.3%, respectively, and their specific activities were 23.4, 21.6, and 30.1 GBq/µg (0.63, 0.58, and 0.81 kCi/µg), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Nakamoto et al. analyzed the binding abilities of ^125^I-Bt-MLS128 and ^125^I-SA to the immobilized avidin, biotin, and LS180 tumor cells by incubating them together for 1 h at 4ºC (22). More than 95% of ^125^I-Bt-MLS128 bound to the immobilized avidin. The immunoreactive fraction of ^125^I-Bt-MLS128 that bound to the LS180 tumor cells was 47.2%, which was slightly lower than that of the unmodified MLS128 (data not shown). ^125^I-SA showed >90% binding to the biotin-coated beads. ^125^I-Bt-OST6 showed no significant binding with the LS180 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Zhang et al. from the same research group as Nakamoto et al. investigated the biodistribution of the Bt-MLS128-^125^I-SA system in female BALB/c nu/nu mice bearing intraperitoneal LS180 tumor xenografts (4, 5). They first analyzed the biodistribution of ^125^I-Bt-MLS128 at 48 h after injection via intraperitoneal (i.p.) or intravenous (i.v.) routes (n = 5 mice/group). There was no difference in tumor uptake or tumor/nontumor ratios between i.p. and i.v. administration of the ^125^I-Bt-MLS128. The tumor uptake levels were 23.69 ± 5.83 and 23.81 ± 5.83% injected dose per gram tissue (ID/g) for i.p. and i.v., respectively. The tumor/blood ratios were 2.07 and 2.36 for i.p. and i.v., respectively. They were then analyzed the biodistribution of ^125^I-SA in two-step targeting experiments. The mice were pretreated with Bt-MLS128, and 2 days later they were injected with ^125^I-SA via different routes (i.p. and i.v.) (n = 4 mice/group) and with different doses (n = 4–6 mice/group). The mice were euthanized 6 h after injection of ^125^I-SA. For the control mice, Bt-MLS128 was replaced by Bt-OST6. The analysis showed that the tumor uptake of ^125^I-SA and the tumor/blood ratio of the radioactivity were significantly higher in the mice given ^125^I-SA via i.p. injection than via i.v. injection (P < 0.05), regardless of the administration routes of Bt-MLS128. The difference remained significant up to 48 h. For the i.p. route, the radioactivity levels in the tumors were 16.53 ± 3.03, 15.33 ± 1.90, and 13.17 ± 3.18% injected dose per gram tissue (ID/g), and the tumor/blood ratios of the radioactivity were 1.52, 3.04, and 5.06, at 6, 24, and 48 h, respectively. For the i.v. route, the radioactivity levels in the tumors were 7.66 ± 1.87, 8.72 ± 1.46, and 9.04 ± 2.33% ID/g, and the tumor/blood ratios of the radioactivity were 0.78, 1.66, and 2.96, at 6, 24, and 48 h, respectively. ^125^I-SA doses increasing from 5 µg to 50 µg decreased the tumor uptake (P = 0.005) but not the tumor/blood ratios (P = 0.585). With i.p. route, the radioactivity levels in the tumors were 32.13 ± 4.00 and 20.89 ± 1.68% ID/g, and the tumor/blood ratios of the radioactivity were 1.53 and 1.45 at 5 µg and 50 µg, respectively. The administration routes for Bt-MLS128 did not result in a significant difference in either the tumor uptake or the tumor/blood ratio (i.p. versus i.v., P > 0.05). Increase of Bt-MLS128 doses from 50 µg to 300 µg led to increased tumor uptake (P = 0.002), but once again the tumor/blood ratio remained unchanged (P = 0.337). Without the Bt-MLS128 pretreatment, the tumor uptake of the i.p. injections of ^125^I-SA was significantly lower: 6.45 and 3.75% ID/g at 6 and 24 h, respectively (P < 0.05), which represents non-specific binding.

Autoradiography of the ex vivo tumors showed a higher uptake in the margin than in the center of the tumors with the i.p. route, but a more uniform intratumoral distribution with the i.v. route (5). By increasing the dose, ^125^I-SA penetrated more deeply into the tumor tissue. The investigators concluded that there was no difference in the biodistribution of ^125^I-SA between i.v. and i.p. pretargeting with Bt- MLS128, and that the i.p. route of ^125^I-SA administration resulted in a higher tumor uptake and tumor/blood ratio than the i.v. route. The investigators also concluded that a higher dose of Bt-MLS128 led to higher tumor uptake of ^125^I-SA, but a higher dose of ^125^I-SA led to lower tumor uptake of ^125^I-SA.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Springer G.F. (1997). Immunoreactive T and Tn epitopes in cancer diagnosis, prognosis, and immunotherapy. J Mol Med.
2 Ando H., Matsushita T., Wakitani M., Sato T., Kodama-Nishida S., Shibata K., Shitara K., Ohta S. (2008). Mouse-human chimeric anti-Tn IgG1 induced anti-tumor activity against Jurkat cells in vitro and in vivo. Biol Pharm Bull.
3 Li Q., Anver M.R., Butcher D.O., Gildersleeve J.C. (2009). Resolving conflicting data on expression of the Tn antigen and implications for clinical trials with cancer vaccines. Mol Cancer Ther.
4 Zhang M., Yao Z., Sakahara H., Saga T., Nakamoto Y., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Effect of administration route and dose of streptavidin or biotin on the tumor uptake of radioactivity in intraperitoneal tumor with multistep targeting. Nucl Med Biol.
5 Zhang M., Yao Z., Saga T., Sakahara H., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1998). Improved intratumoral penetration of radiolabeled streptavidin in intraperitoneal tumors pretargeted with biotinylated antibody. J Nucl Med.
6 Zhang M., Sakahara H., Yao Z., Saga T., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1997). Intravenous avidin chase improved localization of radiolabeled streptavidin in intraperitoneal xenograft pretargeted with biotinylated antibody. Nucl Med Biol.
7 Yao Z., Zhang M., Kobayashi H., Sakahara H., Nakada H., Yamashina I., Konishi J. (1995). Improved targeting of radiolabeled streptavidin in tumors pretargeted with biotinylated monoclonal antibodies through an avidin chase. J Nucl Med.
8 Becker J.M., Wilchek M. (1972). Inactivation by avidin of biotin-modified bacteriophage. Biochim Biophys Acta.
9 Hsu S.M., Raine L., Fanger H. (1981). Use of avidin-biotin-peroxidase complex (ABC) in immunoperoxidase techniques: a comparison between ABC and unlabeled antibody (PAP) procedures. J Histochem Cytochem.
10 Babino A., Oppezzo P., Bianco S., Barrios E., Berois N., Navarrete H., Osinaga E. (2000). Tn antigen is a pre-cancerous biomarker in breast tissue and serum in n-nitrosomethylurea-induced rat mammary carcinogenesis. Int J Cancer.
11 Hakomori S. (2001). Tumor-associated carbohydrate antigens defining tumor malignancy: basis for development of anti-cancer vaccines. Adv Exp Med Biol.
12 Kulkarni K.A., Sinha S., Katiyar S., Surolia A., Vijayan M., Suguna K. (2005). Structural basis for the specificity of basic winged bean lectin for the Tn-antigen: a crystallographic, thermodynamic and modelling study. FEBS Lett.
13 Kurtenkov O., Klaamas K., Rittenhouse-Olson K., Vahter L., Sergejev B., Miljukhina L., Shljapnikova L. (2005). IgG immune response to tumor-associated carbohydrate antigens (TF, Tn, alphaGal) in patients with breast cancer: impact of neoadjuvant chemotherapy and relation to the survival. Exp Oncol.
14 Lescar J., Sanchez J.F., Audfray A., Coll J.L., Breton C., Mitchell E.P., Imberty A. (2007). Structural basis for recognition of breast and colon cancer epitopes Tn antigen and Forssman disaccharide by Helix pomatia lectin. Glycobiology.
15 Dausset J., Moullec J., Bernard J. (1959). Acquired hemolytic anemia with polyagglutinability of red blood cells due to a new factor present in normal human serum (Anti-Tn). Blood.
16 Springer G.F., Desai P.R., Spencer B.D., Tegtmeyer H., Carlstedt S.C., Scanlon E.F. (1995). T/Tn antigen vaccine is effective and safe in preventing recurrence of advanced breast carcinoma. Cancer Detect Prev.
17 Slovin S.F., Ragupathi G., Musselli C., Olkiewicz K., Verbel D., Kuduk S.D., Schwarz J.B., Sames D., Danishefsky S., Livingston P.O., Scher H.I. (2003). Fully synthetic carbohydrate-based vaccines in biochemically relapsed prostate cancer: clinical trial results with alpha-N-acetylgalactosamine-O-serine/threonine conjugate vaccine. J Clin Oncol.
18 Cipolla L., Rescigno M., Leone A., Peri F., La Ferla B., Nicotra F. (2002). Novel Tn antigen-containing neoglycopeptides: synthesis and evaluation as anti tumor vaccines. Bioorg Med Chem.
19 Takahashi H.K., Metoki R., Hakomori S. (1988). Immunoglobulin G3 monoclonal antibody directed to Tn antigen (tumor-associated alpha-N-acetylgalactosaminyl epitope) that does not cross-react with blood group A antigen. Cancer Res.
20 Yao Z., Sakahara H., Zhang M., Kobayashi H., Nakada H., Yamashina I., Konishi J. (1995). Radioimmunoimaging of colon cancer xenografts with anti-Tn monoclonal antibody. Nucl Med Biol.
21 Yao Z., Zhang M., Sakahara H., Saga T., Kobayashi H., Nakamoto Y., Toyama S., Konishi J. (1998). Increased streptavidin uptake in tumors pretargeted with biotinylated antibody using a conjugate of streptavidin-fab fragment. Nucl Med Biol.
22 Nakamoto Y., Saga T., Sakahara H., Yao Z., Zhang M., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Three-step tumor imaging with biotinylated monoclonal antibody, streptavidin and 111In-DTPA-biotin. Nucl Med Biol.
23 Numata Y., Nakada H., Fukui S., Kitagawa H., Ozaki K., Inoue M., Kawasaki T., Funakoshi I., Yamashina I. (1990). A monoclonal antibody directed to Tn antigen. Biochem Biophys Res Commun.
24 Oppezzo P., Osinaga E., Tello D., Bay S., Cantacuzene D., Irigoin F., Ferreira A., Roseto A., Cayota A., Alzari P., Pritsch O. (2000). Production and functional characterization of two mouse/human chimeric antibodies with specificity for the tumor-associated Tn-antigen. Hybridoma.